# AlexaFluor 488-conjugated antibody against lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)

Chemical name: | AlexaFluor 488-conjugated antibody against lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)
Abbreviated name: | Alexa488-Anti-LYVE-1
Synonym:
Agent category: | Antibody
Target: | Lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1)
Target category: | Receptor
Method of detection: | Optical, fluorescence imaging
Source of signal/contrast: | AlexaFluor 488
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LYVE-1)]

The primary function of the lymphatic system is to drain ~10% of the interstitial fluid from small capillaries to lymphatic vessels through lymph nodes (LNs) and finally to the venous system (1-5). LNs form a natural filter for lymphatic drainage and prevent the possible migration of cancer cells from the lymphatic system into the body. As the first LN that receives lymph drainage from a tumor bed, the sentinel LN is very likely to contain cancer cells if the primary tumor has spread via the lymphatic system (1, 2). The lymphatic system is complex, and its detection and mapping remain challenging (1, 2, 6, 7). However, with advances of new imaging agents and techniques, imaging and mapping of both the lymphatic vessels and the LNs are now possible with x-ray–computed tomography, ultrasound, nuclear medicine, and magnetic resonance imaging (7-9). There is increasing evidence that tumor cells induce lymphangiogenesis in tumor-draining LNs in experimental models of cancer (10, 11) as well as in LNs of patients with metastatic melanoma and breast cancer (12, 13). Therefore, LN lymphangiogenesis might provide a target to image the early stages of tumor metastasis. In addition, chronic inflamed tissues produce vascular endothelial growth factor to induce lymphangiogenesis in draining LNs.

Hyaluronan (HA) is an abundant extracellular matrix glycosaminoglycan in skin and mesenchymal tissues, where it facilitates cell migration during inflammation, wound healing, metastasis, and embryonic morphogenesis (14, 15). CD44 is an integral cell membrane glycoprotein on leukocytes and has an important role in matrix adhesion lymphocyte activation and LN homing (16). CD44 binds HA to induce extravasation of lymphoid cells. Lymphatic vessel endothelial hyaluronan receptor-1 (LYVE-1) has a 41% homology to CD44, and LYVE-1 expression is largely restricted to endothelial cells of lymphatic vessels and splenic sinusoidal endothelial cells. Expression was undetectable on lymphocytes, hematopoietic cells, or vascular endothelial cells. McElroy et al. (17) used AlexaFluor 488-conjugated antibody against LYVE-1 (Alexa488-anti-LYVE-1) for in vivo fluorescence imaging of lymphatic vessels and tumor cell trafficking.

### Related Resource Links:

- Chapters in MICAD (LYVE-1 (http://www.ncbi.nlm.nih.gov/books?term=LYVE-1%20AND%20micad%5Bbook%5D), CD44 (http://www.ncbi.nlm.nih.gov/books?term=CD44%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (LYVE-1 (http://www.ncbi.nlm.nih.gov/gene/10894), CD44 (http://www.ncbi.nlm.nih.gov/gene/960))
- Articles in Online Mendelian Inheritance in Man (OMIM) (LYVE-1 (http://www.ncbi.nlm.nih.gov/omim/605702), CD44 (http://www.ncbi.nlm.nih.gov/omim/107269))
- Clinical trials (LYVE-1 (http://www.clinicaltrials.gov/ct2/show/NCT00748657?term=LYVE1&rank=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor%20LYVE-1%20AND+synthesis)]

Anti-mouse LYVE-1 rat antibody (6.6 nmol, clone 223322, R&D Systems) was conjugated with AlexaFluor 488 tetrafluorophenyl ester in sodium bicarbonate buffer (pH 8) for 60 min at room temperature (17). Alexa488-anti-LYVE-1 was purified on a column by centrifugation. Control Alexa488-IgG was prepared similarly. There were approximately four dye moieties per antibody. Alexa488-anti-LYVE-1 immunoreactivity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor%20LYVE-1%20AND+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor%20LYVE-1+AND+rodentia)]

McElroy et al. (17) injected ~0.02 nmol Alexa488-anti-LYVE-1 into tissues around the mammary inguinal LN in nude mice (n = 3). The inguinal LN, draining lymphatics, and axillary LN were imaged using a small-animal fluorescence imaging system at 0, 4, 12, 24, 36, 48, and 72 h after injection. A clear signal was obtained in the inguinal LN, draining lymphatics, and axillary LN at 4 h, and it was still detectable at 48 h. Control Alexa488-IgG showed minimal signal in the draining lymphatics at 4 h after injection and no signal at 12 h after injection. Immunostaining of lymphatic tissue showed that Alexa488-anti-LYVE-1 was localized to lymphatic endothelium, whereas no signal was observed in the adjacent arteries and veins. Human XPA-1 pancreatic cancer cells transfected with red fluorescent protein (2 × 10^6^ cells) were injected into the tissue around the mammary inguinal LN in nude mice (n = 6) 4 h after injection of Alexa488-anti-LYVE-1. The tumor cells expressing the red fluorescent protein were clearly visible within the lymphatic vessels trafficking from the inguinal LN to the axillary LN in all six mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor%20LYVE-1+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor%20LYVE-1+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor%20LYVE-1%20AND+human)]

No publication is currently available.

## NIH Support

CA099258, CA103563, R01, CA109949-01

## References

1 Clement O., Luciani A. (2004). Imaging the lymphatic system: possibilities and clinical applications. Eur Radiol.
2 Styblo T., Aarsvold J.N., Grant S.F., Cohen C., Larsen T., Waldrop S., Alazraki N.P. (2001). Sentinel lymph nodes: optimizing success. Semin Roentgenol.
3 Hoh C.K., Wallace A.M., Vera D.R. (2003). Preclinical studies of [(99m)Tc]DTPA-mannosyl-dextran. Nucl Med Biol.
4 Salem C.E., Hoh C.K., Wallace A.M., Vera D.R. (2006). A preclinical study of prostate sentinel lymph node mapping with [99mTC]diethylenetetramine pentaacetic acid-mannosyl-dextran. J Urol.
5 Vera D.R., Wallace A.M., Hoh C.K., Mattrey R.F. (2001). A synthetic macromolecule for sentinel node detection: (99m)Tc-DTPA-mannosyl-dextran. J Nucl Med.
6 Torabi M., Aquino S.L., Harisinghani M.G. (2004). Current concepts in lymph node imaging. J Nucl Med.
7 Schoder H., Glass E.C., Pecking A.P., Harness J.K., Wallace A.M., Hirnle P., Alberini J.L., Vilain D., Larson S.M., Hoh C.K., Vera D.R. (2006). Molecular targeting of the lymphovascular system for imaging and therapy. Cancer Metastasis Rev.
8 Luciani A., Itti E., Rahmouni A., Meignan M., Clement O. (2006). Lymph node imaging: basic principles. Eur J Radiol.
9 Wunderbaldinger P. (2006). Problems and prospects of modern lymph node imaging. Eur J Radiol.
10 Qian C.N., Berghuis B., Tsarfaty G., Bruch M., Kort E.J., Ditlev J., Tsarfaty I., Hudson E., Jackson D.G., Petillo D., Chen J., Resau J.H., Teh B.T. (2006). Preparing the "soil": the primary tumor induces vasculature reorganization in the sentinel lymph node before the arrival of metastatic cancer cells. Cancer Res.
11 Harrell M.I., Iritani B.M., Ruddell A. (2007). Tumor-induced sentinel lymph node lymphangiogenesis and increased lymph flow precede melanoma metastasis. Am J Pathol.
12 Dadras S.S., Lange-Asschenfeldt B., Velasco P., Nguyen L., Vora A., Muzikansky A., Jahnke K., Hauschild A., Hirakawa S., Mihm M.C., Detmar M. (2005). Tumor lymphangiogenesis predicts melanoma metastasis to sentinel lymph nodes. Mod Pathol.
13 Van den Eynden G.G., Vandenberghe M.K., van Dam P.J., Colpaert C.G., van Dam P., Dirix L.Y., Vermeulen P.B., Van Marck E.A. (2007). Increased sentinel lymph node lymphangiogenesis is associated with nonsentinel axillary lymph node involvement in breast cancer patients with a positive sentinel node. Clin Cancer Res.
14 Jiang D., Liang J., Noble P.W. (2011). Hyaluronan as an immune regulator in human diseases. Physiol Rev.
15 Sironen R.K., Tammi M., Tammi R., Auvinen P.K., Anttila M., Kosma V.M. (2011). Hyaluronan in human malignancies. Exp Cell Res.
16 Aruffo A., Stamenkovic I., Melnick M., Underhill C.B., Seed B. (1990). CD44 is the principal cell surface receptor for hyaluronate. Cell.
17 McElroy M., Hayashi K., Garmy-Susini B., Kaushal S., Varner J.A., Moossa A.R., Hoffman R.M., Bouvet M. (2009). Fluorescent LYVE-1 antibody to image dynamically lymphatic trafficking of cancer cells in vivo. J Surg Res.